# ^68^Ga-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-2-(2-nitroimidazolyl)ethylamine

Chemical name: | ^68^Ga-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-2-(2-nitroimidazolyl)ethylamine
Abbreviated name: | ^68^Ga-DOTA-NI, ^68^Ga-4
Synonym:
Agent Category: | Compound
Target: | Hypoxic tissue
Target Category: | Hypoxia
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^68^Ga
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DOTA-Nitroimidazole)]

Hypoxia is found in a variety of solid tumors and leads to tumor progression and resistance to chemotherapy and radiotherapy (1, 2). Tumor oxygenation is heterogeneously distributed within human tumors (3). It would be beneficial to assess tumor oxygenation before and after therapy to provide an evaluation of tumor response to treatment and an insight into new therapeutic treatments (4). Tumor oxygenation is measured invasively using computerized, polarographic, oxygen-sensitive electrodes, which is regarded as the gold standard (5). Functional and noninvasive imaging of intratumoral hypoxia has been demonstrated to be feasible for the measurement of tumor oxygenation (6).

Chapman proposed the use of 2-nitroimidazole compounds for hypoxia imaging in 1979 (7). 2-Nitroimidazole compounds are postulated to undergo reduction in hypoxic conditions, forming highly reactive oxygen radicals that subsequently bind covalently to macromolecules inside the cells (8). In normoxic conditions, the reduced molecule is rapidly reoxidized and transported from the cell. [^18^F]Fluoromisonidazole ([^18^F]FMISO (http://www.ncbi.nlm.nih.gov/bookshelf/br.fcgi?book=micad&part=FMISO)) is the most widely used positron emission tomography (PET) tracer for imaging tumor hypoxia (6). However, it has slow clearance kinetics and a high lipophilicity, resulting in substantial background in PET scans. [^18^F]Fluoroazomycinarabinofuranoside ([^18^F]FAZA (http://www.ncbi.nlm.nih.gov/books/NBK23282/)) is a 2-nitroimidazole with a sugar addition (9) and has been studied as a hypoxia-imaging agent, showing promising results in various tumor models in rats and mice (10, 11). ^68^Ga-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-2-(2-nitroimidazolyl)ethylamine (^68^Ga-DOTA-NI, ^68^Ga-4) and ^68^Ga-isothiocyanatobenzyl-tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-2-(2-nitroimidazolyl)ethylamine (^68^Ga-SCN-Bz-DOTA-NI, ^68^Ga-5) were prepared for hypoxic tissue imaging (12).

### Related Resource Links:

- Chapters in MICAD (Hypoxia (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=Hypoxia+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (Hypoxia-inducible factor 1, alpha subunit (http://www.ncbi.nlm.nih.gov/sites/entrez?db=gene&cmd=Retrieve&dopt=full_report&list_uids=3091))
- Articles in Online Mendelian Inheritance in Man (OMIM) (Hypoxia (http://www.ncbi.nlm.nih.gov/omim?Db=omim&Cmd=DetailsSearch&Term=hypoxia%5BAll+Fields%5D))
- Clinical trials (Hypoxia imaging (http://www.clinicaltrials.gov/ct2/results?term=hypoxia+imaging))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DOTA-Nitroimidazole%20and%20synthesis)]

Hoigebazar et al. (12) synthesized two nitroimidazole derivatives by conjugating nitroimidazole and DOTA via an amide bond and a thiourea bond. A solution mixture of 2-(2-nitroimidazolyl)ethylamine (0.08 mmol) and DOTA (0.12 mmol) was incubated overnight at room temperature to yield DOTA-2-(2-nitroimidazolyl)ethylamine employing an amide bond linkage (DOTA-NI, 4). DOTA-NI was purified with high-performance liquid chromatography. To label with ^68^Ga, a mixture of DOTA-NI and ^68^GaCl_3_ was heated in acetate buffer (pH 3) for 10 min at 100°C. ^68^Ga-DOTA-NI was purified with cartridge filtration. Labeling yields were >98%. ^68^Ga-SCN-Bz-DOTA-NI was prepared similarly using a thiourea bond linkage with labeling yields of >98%. Both agents were stable at room temperature for 2 h with low protein binding. ^68^Ga-DOTA-NI and ^68^Ga-SCN-Bz-DOTA-NI are hydrophilic and have low partition coefficients (log P) of −4.6 and −4.5, respectively. The specific activities of ^68^Ga-DOTA-NI and ^68^Ga-SCN-Bz-DOTA-NI were 4.81 GBq/nmol (0.13 Ci/nmol) and 7.77 GBq/nmol (0.21 Ci/nmol), respectively.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DOTA-Nitroimidazole%20and%20in%20vitro)]

In vitro studies indicated that uptake values of both ^68^Ga-DOTA-NI and ^68^Ga-SCN-Bz-DOTA-NI in cells from the Hela human cell line and the CT-26 mouse colon cell line were significantly higher (n = 4, P < 0.05) under hypoxic conditions for 4 h than under normoxic conditions after 60 min of incubation (2.4 times in Hela cells, 6.8 times in CT-26 cells for ^68^Ga-DOTA-NI; 2.1 times in Hela cells, 3.4 times in CT-26 cells for ^68^Ga-SCN-Bz-DOTA-NI) (12).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DOTA-Nitroimidazole%20and%20rodentia)]

Ex vivo biodistribution studies of ^68^Ga-DOTA-NI and ^68^Ga-SCN-Bz-DOTA-NI in mice (n = 4/group) bearing CT-26 tumors exhibited rapid clearance of the tracer from the body over time (10, 30, 60, and 120 min after injection) (12). The highest uptake values were found in the kidneys, with ~10% injected dose/gram (ID/g) for ^68^Ga-DOTA-NI and ~15% ID/g for ^68^Ga-SCN-Bz-DOTA-NI at 10 min after injection. The liver and intestine accumulation values of ^68^Ga-SCN-Bz-DOTA-NI at 60 min (~3% ID/g, respectively) were higher than those of ^68^Ga-DOTA-NI (~1% ID/g, respectively) at the same time point. The initial tumor uptake values for ^68^Ga-DOTA-NI and ^68^Ga-SCN-Bz-DOTA-NI at 10 min after injection were 3.17% ID/g and 2.78% ID/g , respectively. These radioactivity levels declined over time for both tracers. The tumor/muscle ratios for ^68^Ga-DOTA-NI and ^68^Ga-SCN-Bz-DOTA-NI, which were ~0.65, at 60 min after injection were lower than those for [^18^F]FAZA (3.27) and [^18^F]FMISO (1.19) at the same time point, whereas the tumor/muscle ratios for ^68^Ga-DOTA-NI (~3.5) and ^68^Ga-SCN-Bz-DOTA-NI (~3.5) at 60 min after injection were higher than those for [^18^F]FAZA (1.7) and [^18^F]FMISO (1.7) at the same time point (13).

Tumor standardized uptake values (SUVs) at 30 min and 60 min after injection for ^68^Ga-DOTA-NI (0.81 ± 0.10 and 0.53 ± 0.10, respectively) and ^68^Ga-SCN-Bz-DOTA-NI (0.31 ± 0.10 and 0.17 ± 0.10, respectively) were determined with PET imaging in mice bearing CT-26 tumors (12). The tumor SUV/muscle SUV ratios of ^68^Ga-DOTA-NI were 5.08 ± 2.2 and 5.64 ± 0.8 at 30 min and 60 min, respectively. The tumor SUV/muscle SUV ratios of ^68^Ga-SCN-Bz-DOTA-NI were 1.86 ± 0.3 and 3.83 ± 0.8 at 30 min and 60 min, respectively. Both tracers showed high accumulation in the kidneys and urinary bladder.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DOTA-Nitroimidazole%20and%20%28dog%20or%20pig%20or%20cat%20or%20rabbit%20or%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DOTA-Nitroimidazole%20and%20primate%20not%20human)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DOTA-Nitroimidazole%20and%20humans)]

No publication is currently available.

## References

1 Rajendran J.G., Krohn K.A. (2005). Imaging hypoxia and angiogenesis in tumors. Radiol Clin North Am.
2 Vaupel P., Mayer A. (2005). Hypoxia and anemia: effects on tumor biology and treatment resistance. Transfus Clin Biol.
3 Vaupel P., Harrison L. (2004). Tumor hypoxia: causative factors, compensatory mechanisms, and cellular response. Oncologist.
4 Dehdashti F., Grigsby P.W., Mintun M.A., Lewis J.S., Siegel B.A., Welch M.J. (2003). Assessing tumor hypoxia in cervical cancer by positron emission tomography with 60Cu-ATSM: relationship to therapeutic response-a preliminary report. Int J Radiat Oncol Biol Phys.
5 Raleigh J.A., Dewhirst M.W., Thrall D.E. (1996). Measuring Tumor Hypoxia. Semin Radiat Oncol.
6 Foo S.S., Abbott D.F., Lawrentschuk N., Scott A.M. (2004). Functional imaging of intratumoral hypoxia. Mol Imaging Biol.
7 Chapman J.D. (1979). Hypoxic sensitizers--implications for radiation therapy. N Engl J Med.
8 Chapman J.D., Baer K., Lee J. (1983). Characteristics of the metabolism-induced binding of misonidazole to hypoxic mammalian cells. Cancer Res.
9 Reischl G., Ehrlichmann W., Bieg C., Solbach C., Kumar P., Wiebe L.I., Machulla H.J. (2005). Preparation of the hypoxia imaging PET tracer [18F]FAZA: reaction parameters and automation. Appl Radiat Isot.
10 Piert M., Machulla H.J., Picchio M., Reischl G., Ziegler S., Kumar P., Wester H.J., Beck R., McEwan A.J., Wiebe L.I., Schwaiger M. (2005). Hypoxia-specific tumor imaging with 18F-fluoroazomycin arabinoside. J Nucl Med.
11 Sorger D., Patt M., Kumar P., Wiebe L.I., Barthel H., Seese A., Dannenberg C., Tannapfel A., Kluge R., Sabri O. (2003). [18F]Fluoroazomycinarabinofuranoside (18FAZA) and [18F]Fluoromisonidazole (18FMISO): a comparative study of their selective uptake in hypoxic cells and PET imaging in experimental rat tumors. Nucl Med Biol.
12 Hoigebazar L., Jeong J.M., Hong M.K., Kim Y.J., Lee J.Y., Shetty D., Lee Y.S., Lee D.S., Chung J.K., Lee M.C. (2011). Synthesis of 68Ga-labeled DOTA-nitroimidazole derivatives and their feasibilities as hypoxia imaging PET tracers. Bioorg Med Chem.
13 Hoigebazar L., Jeong J.M., Choi S.Y., Choi J.Y., Shetty D., Lee Y.S., Lee D.S., Chung J.K., Lee M.C., Chung Y.K. (2010). Synthesis and characterization of nitroimidazole derivatives for 68Ga-labeling and testing in tumor xenografted mice. J Med Chem.